# ^125^I-Labeled murine anti-CD20 antigen monoclonal antibody NuB2 conjugated to one or three octaarginine (maleimide-(6-aminocaproic acid)_2_-(D-Arg)_8_-(D-Tyr)) peptide chains

Chemical name: | ^125^I-Labeled murine anti-CD20 antigen monoclonal antibody NuB2 conjugated to one or three octaarginine (maleimide-(6-aminocaproic acid)_2_-(D-Arg)_8_-(D-Tyr)) peptide chains
Abbreviated name: | [^125^I]SIB-NuB2I and [^125^I]SIB-NuB2III
Synonym:
Agent Category: | Monoclonal antibody
Target: | CD20 antigen
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The B cell differentiation antigen CD20 is a transmembrane, non-glycosylated, hydrophobic protein that is characteristically expressed in >90% of non-Hodgkin lymphoma tumors. Although the exact function(s) of CD20 in the cell are not known, CD20 is believed to play a role in B cell growth, activation, and maintenance of cellular calcium homeostasis (1). In addition, depletion of B cells with anti-CD20 monoclonal antibodies (mAbs) in human CD20/non-obese diabetic mice has been shown to prevent and reverse diabetes in the animals (2). Also, once an antibody (Ab) binds to an extracellular domain of the CD20, the Ab-antigen complex is not internalized and expression of the antigen on the cell surface is not downregulated (3). Because of its specific presence on non-Hodgkin lymphoma tumor cells, the antigen is a therapeutic target of different anti-CD20 Abs, such as rituximab (http://www.cancer.gov/cancertopics/druginfo/rituximab) for monotherapy or combination therapy with a chemotherapeutic agent, or tositumomab (http://us.gsk.com/products/assets/us_bexxar.pdf) (^131^I-labeled) or ibritumomab (http://www.cancer.gov/drugdictionary/?CdrID=38483) (^90^Y-conjugated) for radioimmunotherapy (RIT), all of which are approved by the United States Food and Drug Administration for the treatment of this disease (4). In general, radionuclide-labeled Abs are used to detect or monitor cancer progression and treatment with positron emission tomography and single-photon emission computed tomography (SPECT); however, due to prolonged blood circulation and slow clearance of the radiolabeled macromolecules (~150 kDa in size) from the system, longer waiting times are required before target/background signal (T/B) ratios reduce to suitable levels for investigators to diagnose or monitor ailments with non-invasive imaging techniques (5, 6). It is also known that, due to their large size, Abs exhibit limited penetration and accumulation in lesions, which results in a low efficacy of the radiolabeled Abs against solid tumors (7). Hence, increasing the accumulation and retention of a radiolabeled Ab in tumors can not only improve the success rate of RIT but can also produce higher T/B ratios and generate good images to diagnose or monitor cancers.

Investigators have shown that co-injection of a cell penetration peptide (CPP) with a divalent single-chain Fv Ab fragment facilitates increased uptake and retention of the radio-biochemical by solid tumors (8). In other studies, arginine-rich, CPP-conjugated, radiolabeled Abs were shown to accumulate only in cultured cells, but no uptake of the construct was observed in tumors cells under in vivo conditions (7). Miyamoto et al. reported enhanced accumulation of Abs modified to contain multivalent binding domains in tumors, which suggests that such modifications can promote increased Ab-antigen binding and enhance the cellular retention of Ab tracers (7). On the basis of these observations, Miyamoto et al. conjugated an octaarginine peptide (maleimide-(6-aminocaproic acid)_2_-(D-Arg)_8_-(D-Tyr); R_8_) to NuB2, a murine anti-CD20 mAb, to evaluate the use of a membrane-anchoring peptide for the enhancement of Ab-antigen interaction and cellular retention (7). Two separate R_8_-NuB2 conjugates containing either one (NuB2I) or three (NuB2III) R_8_ chains were produced by the investigators. The complexes were then labeled with [^125/131^I]-N-succinimidyl 3-indobenzoate (SIB) to obtain [^125/131^I]-SIB-NuB2I and [^125^I]-SIB-NuB2III, respectively, and the conjugates were characterized in vitro. The biodistribution of both labeled mAbs was subsequently studied in normal mice and severe combined immunodeficiency (SCID) mice bearing RPMI 1788 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-156&Template=cellBiology) tumors. This chapter describes the results obtained from studies performed with the [^125/131^I]-SIB-NuB2I and [^125^I]-SIB-NuB2III mAbs.

### Other Sources of Information

- Other CD20-imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=anti-CD20%20AND%20micad%5bbook%5d)
- Clinical trials (http://clinicaltrials.gov/ct2/results?term=anti+CD-20+antibodies&pg=1) with anti-CD20 antibodies
- Human CD20 protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_031457.1)
- CD20 information in Entrez Gene (http://www.ncbi.nlm.nih.gov/nuccore?Db=gene&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_gene&IdsFromResult=13899294) (Gene ID: 83661)
- Information on CD20 in Online Mendelian Inheritance in Man (OMIM) Database (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=gene&Cmd=Link&LinkName=gene_omim&LinkReadableName=OMIM&IdsFromResult=83661)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20antibody%20synthesis&cmd=DetailsSearch)]

The NuB2 murine mAb used for studies described in this chapter was supplied by a commercial laboratory (7). The R_8_ peptide was synthesized on an automated peptide synthesizer, and the two NuB2 conjugates (NuB2I and NuB2III) were prepared as described by Miyamoto et al. (7). The number of R_8_ molecules bound to NuB2I and NuB2III were determined to be 0.92 and 3.38, respectively. The NuB2I and NuB2III were then radiolabeled with ^125/131^I using [^125/131^I]-SIB as detailed elsewhere (7). In some studies, [^125^I]-NuB2 (prepared by direct iodination of the mAb with the chloramines T method) was used for comparison purposes (7). The radiochemical purity of the [^125/131^I]-SIB–labeled mAbs and [^125^I]-NuB2 was >95% and 99%, respectively, as determined with size-exclusion high-performance liquid chromatography and thin-layer chromatography. Nonradioactive SIB conjugates of NuB2, NuB2I, and NuB2III were also prepared for use in some studies. The stability and specific activity of the various radiolabeled mAbs were not reported.

The NuB2, NuB2I, and NuB2III mAbs were also labeled with Alexa Fluor 488 (AF) to generate AF-labeled mAbs for use in some studies. Approximately four AF molecules were reported to be linked to each molecule of the various AF-mAbs (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20monoclonal%20antibody%20NuB2I%20in%20vitro%20studies&cmd=DetailsSearch)]

In a confocal microscopy study using the AF-labeled mAbs with RPMI 1788 cells, the green fluorescent mAbs were shown to be present only on the outer surface of the cell membranes, indicating that the tracers were not internalized by the cells (7).

The immunoreactivity of the nonradioactive SIB-NuB2, SIB-NuB2I, SIB-NuB2III, and the different AF-mAb conjugates was evaluated in a [^125^I]-NuB2 mAb binding assay with RPMI 1788 cells, which have a high expression of the CD20 antigen (7). All of the unlabeled mAb conjugates were reported to show similar binding inhibition curves. The presence of excess nonradioactive NuB2 mAbs in the binding assay almost completely inhibited binding of the [^125^I]-NuB2 mAbs to the cells. This study indicated that the immunoreactivity of all the modified mAbs was similar to that of the parental NuB2 mAb.

The in vitro cell binding and retention of the respective [^125^I]-SIB mAb conjugates were studied using RPMI 1788 cells as described by Miyamoto et al. (7). Compared to [^125^I]-SIB-NuB2, the [^125^I]-SIB-NuB2I and [^125^I]-SIB-NuB2III mAbs were shown to have a 1.4- and 4.3-fold higher binding to the RPMI 1788 cells, respectively. Addition of 1,000-fold excess unlabeled NuB2 to the binding assay resulted in ~80% reduction in the cellular binding of [^125^I]-SIB-NuB2 and [^125^I]-SIB-NuB2I, compared to only ~30% reduction for [^125^I]-SIB-NuB2III. The 50% inhibitory concentrations for the various mAbs were not reported. An investigation of the retention of [^125^I]-SIB-NuB2, [^125^I]-SIB-NuB2I, and [^125^I]-SIB-NuB2III by the RPMI 1788 cells showed that 34.2%, 51.2%, and 61.3%, respectively, of the initial radioactivity from the different conjugates was retained by the cells at 3 h after incubation. From this study, the investigators concluded that the presence of the R_8_ moieties on the NuB2 molecules increased the binding and retention of the modified mAbs on the cell membrane (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20monoclonal%20antibody%20NuB2I%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^]-SIB-NuB2, [^125/131^I I]-SIB-NuB2I, and [^125^I]-SIB-NuB2III was studied in normal and SCID mice bearing RPMI 1788 cell xenograft tumors (7). The three respective [^125^I]-SIB conjugates of NuB2 were administered to normal mice through an intravenous (i.v.) route, and the animals (5 mice/time point) were euthanized at 1, 3, and 24 h postinjection (p.i.). All organs of interest were removed from the mice and weighed, and the accumulated radioactivity in each organ was counted in a gamma counter. Results obtained from this study were presented as percent of injected dose per gram of wet tissue weight (% ID/g). Of the three conjugates, [^125^]-SIB-NuB2 and [^125^I]-SIB-NuB2I showed similar levels of radioactivity in the various organs for the entire duration of the study. The levels of radioactivity at 24 h p.i. for [^125^]-SIB-NuB2 and [^125^I]-SIB-NuB2I were 12.51 ± 0.99% ID/g and 10.54 ± 0.83% ID/g in blood, respectively, 3.54 ± 0.29% ID/g and 2.81 ± 0.40% ID/g in liver, respectively, 3.31 ± 0.15% ID/g and 3.37 ± 0.0.35% ID/g in kidney, respectively, and 1.36 ± 0.33% ID/g and 0.95 ± 0.16% ID/g in the intestine, respectively. The liver/blood (L/B) ratios for the two conjugates were 0.26 ± 0.01 and 0.27 ± 0.03, respectively, at 24 h p.i.. In contrast, the accumulation of label from [^125^I]-SIB-NuB2III was lower in the blood (8.08 ± 0.49% ID/g) and higher in the liver (5.85 ± 0.69% ID/g), but comparable in the kidneys (3.42 ± 0.17% ID/g) and the intestine (0.82 ± 0.17% ID/g) at 24 h p.i. The L/B ratio for [^125^I]-SIB-NuB2III was 0.72 ± 0.05 at 24 h p.i. From these observations, the investigators concluded that radioactivity from [^125^I]-SIB-NuB2III had a significantly (P < 0.01) faster clearance from blood and higher accumulation in the liver than either [^125^]-SIB-NuB2 or [^125^I]-SIB-NuB2I. This also indicated that the number of R_8_ molecules bound to the SIB-NuB2 molecule influenced the in vivo behavior of the mAb conjugates used in this study (7).

Because [^125^]-SIB-NuB2 and [^125^I]-SIB-NuB2I exhibited a similar biodistribution behavior in normal mice, the biodistribution of the two conjugates was studied in SCID mice bearing RPMI 1788 cell xenograft tumors (7). A mixture containing equal amounts of [^125^]-SIB-NuB2 and [^131^I]-SIB-NuB2I (note that NuB2I was labeled with ^131^I and not ^125^I so as to distinguish it from [^125^]-SIB-NuB2) was administerd to the mice as before. The animals were then euthanized at various time points ranging from 24 h to 96 h p.i. to retrieve and determine the amount of radioactivity present in the organs of interest as described above. At 96 h p.i., a significant difference (P < 0.01) was observed in the presence of label from the [^125^]-SIB-NuB2 and [^131^I]-SIB-NuB2I conjugates in the xenograft tumors (4.81 ± 0.78% ID/g and 7.20 ± 1.32% ID/g, respectively) and the liver (1.01 ± 0.10% ID/g and 0.8 ± 0.08% ID/g, respectively). A significant difference (P < 0.05) was apparent in the tumor/blood ratio for the two labeled mAbs (1.59 ± 0.35 and 2.59 ± 0.64, respectively). No difference in the uptake of radioactivity from the two tracers was evident in the kidneys or the intestine. This investigation also suggested that the presence of membrane-anchoring molecule(s) on an antibody can enhance its uptake and retention by an antigen-expressing tumor.

From these studies, the investigators concluded that the conjugation of anchoring molecules such as the octaarginine peptides used in this investigation can be useful to enhance the binding and retention of mAbs for RIT of cancer or other ailments.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20monoclonal%20antibody%20NuB2I%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20monoclonal%20antibody%20NuB2I%20non-human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-CD20%20monoclonal%20antibody%20NuB2I%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Cragg M.S., Walshe C.A., Ivanov A.O., Glennie M.J. (2005). The biology of CD20 and its potential as a target for mAb therapy. Curr Dir Autoimmun.
2 O'Neill S.K., Liu E., Cambier J.C. (2009). Change you can B(cell)eive in: recent progress confirms a critical role for B cells in type 1 diabetes. Curr Opin Endocrinol Diabetes Obes.
3 Parikh S.A., Wierda W.G. (2010). Role of CD20 monoclonal antibodies in previously untreated chronic lymphocytic leukemia. Clin Lymphoma Myeloma Leuk.
4 Bonavida B. (2007). Rituximab-induced inhibition of antiapoptotic cell survival pathways: implications in chemo/immunoresistance, rituximab unresponsiveness, prognostic and novel therapeutic interventions. Oncogene.
5 Olafsen T., Betting D., Kenanova V.E., Salazar F.B., Clarke P., Said J., Raubitschek A.A., Timmerman J.M., Wu A.M. (2009). Recombinant anti-CD20 antibody fragments for small-animal PET imaging of B-cell lymphomas. J Nucl Med.
6 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
7 Miyamoto R., Akizawa H., Nishikawa T., Uehara T., Azuma Y., Nakase I., Futaki S., Hanaoka H., Iida Y., Endo K., Arano Y. (2010). Enhanced target-specific accumulation of radiolabeled antibodies by conjugating arginine-rich peptides as anchoring molecules. Bioconjug Chem.
8 Jain M., Venkatraman G., Batra S.K. (2007). Optimization of radioimmunotherapy of solid tumors: biological impediments and their modulation. Clin Cancer Res.